# ^99m^Tc(CO)_3_-Pyrazolyl-cyclo(Arg-Gly-Asp-D-Tyr-Lys)

Chemical name: | ^99m^Tc- Pyrazolyl-cyclo(Arg-Gly-Asp-D-Tyr-Lys)
Abbreviated name: | ^99m^Tc(CO)_3_-PZ-c(RGDyK)
Synonym:
Agent Category: | Peptide
Target: | Integrin α_v_β_3_
Target Category: | Receptor binding
Method of detection: | SPECT, gamma planar
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mtc+PZ-RGD)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces and mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. Antagonists of α_v_β_3_ are being studied as antitumor and antiangiogenic agents, and the agonists of α_v_β_3_ are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

Most cyclic RGD peptides are composed of five amino acids. Haubner et al. (11) reported that various cyclic RGD peptides exhibit selective inhibition of binding to α_v_β_3_ (inhibition concentration (IC_50_), 7–40 nM) but not to integrins α_v_β_5_ (IC_50_, 600–4,000 nM) or α_IIb_β_3_ (IC_50_, 700–5,000 nM). Various radiolabeled cyclic RGD peptides have been found to have high accumulation in tumors in nude mice (12). The ready availability and low cost of ^99m^Tc led to the development of ^99m^Tc-RGD peptides to target α_v_β_3_ integrins in tumor angiogenesis. ^99m^Tc(CO)_3_-Pyrazolyl-cyclo-(Arg-Gly-Asp-D-Tyr-Lys) (^99m^Tc(CO)_3_-PZ-c(RGDyK)) has been prepared as a single-photon emission computed tomography (SPECT) tracer for imaging α_v_β_3_ integrins in tumors (13).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mtc+PZ-RGD+and+synthesis)]

^99m^Tc(CO)_3_-PZ-c(RGDyK) was prepared by the exchange reaction between [^99m^Tc(H_2_O)_3_(CO)_3_]^+^ and PZ-c(RGDyK) for 60 min at 75°C and purified by high-performance liquid chromatography (13). The radiochemical purity of >98% was obtained and the radiochemical yield was >90%. The specific activity was ~222 GBq/μmol (6 Ci/μmol) at the end of purification.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mtc+PZ-RGD+and+in+vitro)]

Using ^125^I-echistatin in a receptor-binding assay of α_v_β_3_ integrin receptors, Alves et al. (13) reported that c(RGDfV) and PZ-c(RGDyK) had IC_50_ values of 3.68 and 3.01 nM, respectively. Haubner et al. (11) showed that c(RGDyK(SAA)) had IC_50_ values of 20, 4,000, and 3,000 nM for α_v_β_3_, α_v_β_5_, and α_IIb_β_3_, respectively. Cellular uptake of ^99m^Tc-PZ-c(RGDyK) was 1.0 ± 0.09%/mg protein for α_v_β_3_ receptor–positive M21 cells and 0.37 ± 0.11%/mg protein for receptor-negative M21L cells at 37ºC for 90 min. The uptake in M21 cells was reduced to 0.34 ± 0.04%/mg protein by excess c(RGDyK). The in vitro stability of ^99m^Tc-PZ-c(RGDyK) was tested by incubating the radiolabeled peptide in fresh human whole blood at 37ºC for up to 4 h. ^99m^Tc-PZ-c(RGDyK) was >98% intact.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mtc+PZ-RGD+and+rodentia)]

Alves et al. (13) performed biodistribution studies of ^99m^Tc-PZ-c(RGDyK) in nude mice bearing M21 or M21L tumors. The initial tracer accumulation in the α_v_β_3_ integrin–expressing M21 tumor was 2.50 ± 0.29% injected dose per gram (ID/g) at 1 h and decreased to 1.62 ± 0.44% ID/g at 4 h. At 1 h, the highest radioactive concentration was found in the intestines (10.1% ID/g), followed by the liver (8.89% ID/g), kidney (5.65% ID/g), and bone (2.73% ID/g). Blood levels were 0.96% at 1 h and 0.48% at 4 h. The tracer accumulation in the α_v_β_3_ receptor–negative M21L tumor was 0.71 ± 0.08% ID/g at 1 h. The radioactivity levels in other organs were similar to those of mice bearing M21 tumors. The urine contained >75% ID at 1 h. Tumor/blood ratios were 2.6 for M21 tumors and 0.78 for M21L tumors. No blocking experiment was performed. ^99m^Tc-PZ-c(RGDyK) was >98% intact in the liver, serum, and urine at 1 h after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mtc+PZ-RGD+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mtc+PZ-RGD+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mtc+PZ-RGD+and+human)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Haubner R., Wester H.J., Burkhart F., Senekowitsch-Schmidtke R., Weber W., Goodman S.L., Kessler H., Schwaiger M. (2001). Glycosylated RGD-containing peptides: tracer for tumor targeting and angiogenesis imaging with improved biokinetics. J Nucl Med.
12 Chen X., Park R., Shahinian A.H., Tohme M., Khankaldyyan V., Bozorgzadeh M.H., Bading J.R., Moats R., Laug W.E., Conti P.S. (2004). 18F-labeled RGD peptide: initial evaluation for imaging brain tumor angiogenesis. Nucl Med Biol.
13 Alves S., Correia J.D., Gano L., Rold T.L., Prasanphanich A., Haubner R., Rupprich M., Alberto R., Decristoforo C., Santos I., Smith C.J. (2007). In vitro and in vivo evaluation of a novel 99mTc(CO)3-pyrazolyl conjugate of cyclo-(Arg-Gly-Asp-d-Tyr-Lys). Bioconjug Chem.